# S-4-(3-([^11^C]Isopropylamino)-2-hydroxypropoxy)-2H-benzimidazol-2-one

Chemical name: | S-4-(3-([^11^C]isopropylamino)-2-hydroxypropoxy)-2H-benzimidazol-2-one
Abbreviated name: | S-[^11^C]CGP 12388
Synonym: | S-4-(2-Hydroxy-3-[^11^C]propan-2-ylamino-propoxy)benzoimidazol-2-one
Agent category: | Compound
Target: | Peripheral β-adrenoceptors
Target category: | Receptor
Method of detection: | PET
Source of signal: | ^11^C
Activation: | No
Studies: | - In vitro; - Rodents; - Humans | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%5BAll%20Fields%5D%20AND%20%22CGP%2012388%22%5BSubstance%20Name%5D)]

Changes in β-adrenoceptor (G-protein coupled) density and affinity in the heart, lung and brain have been associated with a variety of disorders, such as myocardial ischemia and infarction, congestive heart failure, asthma, chronic obstructive pulmonary disease, depression, schizophrenia, and Alzheimer’s disease (1-3). There are at least four subtypes of β-adrenoceptor receptors: β_1_ to β_4_ (4). Only the β_1_and β_2_-subtypes have been studied extensively. The cardiac receptors are found exclusively in the atria and ventricles and are responsible for the regulation of heart rate and myocardial contractility. The human heart and lung have a β_1_ to β_2_ ratio of 4:1, and 3:7, respectively. In contrast, the cerebral β-adrenoceptors are heterogeneously distributed in the brain with the highest densities in the caudate and putamen, followed by the cortical areas and thalamus. The brain white matter has low densities. β_1_-adrenoceptors are found predominately in the putamen and cortex, while the β_2_-adrenoceptors are found mainly in the hippocampus and cerebellum. The cerebral β-adrenoceptors are implicated in many physiological and behavioral responses.

S-4-(3-(tert-butylamino)-2-hydroxypropoxy)-2H-benzimidazol-one (S-CGP12177) was reported to be an inhibitor of β_1_- and β_2_-adrenoceptors (5). S-[^11^C]CGP 12177 has been studied in vivo by positron emission tomography (PET) producing excellent images of human heart and lung [PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20cgp%2012177%20and%20human)]. However, the synthesis of [^11^C]CGP 12177 was proven to be laborious and often troublesome. Therefore, the isopropyl analogue of S-[^11^C]CGP 12177, S-4-(3-([^11^C]isopropylamino)-2-hydroxypropoxy)-2H-benzimidazol-2-one (S-[^11^C]CGP 12388) is being developed as a PET agent for studying β-adrenoceptors non-invasively in the lung and heart but not the brain since it cannot cross the blood-brain barrier (BBB).

### Related Resource Links:

- Chapters in MICAD (adrenoceptors (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=adrenoceptors%5BAll+Fields%5D+AND+micad%5Bbook%5D))
- Gene information in NCBI (β_1_-adrenoceptor (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=gene&Cmd=DetailsSearch&Term=153%5Buid%5D), β_2_-adrenoceptor (http://www.ncbi.nlm.nih.gov/gene/154))
- Articles in OMIM (β_1_-adrenoceptor (http://omim.org/entry/109630), β_2_-adrenoceptor (http://omim.org/entry/109690))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20CGP%2012388%20and%20synthesis)]

S-[^11^C]CGP 12388 was synthesized via a one-pot reaction of 2-[^11^C]acetone with S-desisopropyl CGP12388 and purified by high-performance liquid chromatography (HPLC) resulted in a radiochemical yield of 18% (end of bombardment) (6). The radiochemical purity was >99.8% with a total synthesis time of 35 min. The specific activity was 22-30 TBq/mmol (600-800 Ci/mmol) at end of synthesis.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20CGP%2012388%20and%20in%20vitro)]

In vitro competition binding studies of [^3^H]CGP 12177 with rat heart membranes produced K_d_ values of 1.74 and 1.67 nM for CGP12388 and CGP 12177 (7), respectively. Using isolated perfused rat heart model with S-[^11^C]CGP 12388 kinetic analysis, the K_d_ values were estimated to be 0.83 ± 0.24 and 1.08 ± 0.31 nM for high-flow group and low-flow group, respectively. B_max_ values were 73 ± 15, 4.0 ± 2.0, and 88 ± 14 fmol/mg protein for the high- and low-flow group, respectively. There was no significant difference in B_max_ and K_d_ between the two groups. Pretreatment of hearts with propranolol (a β-adrenoreceptor antagonist) in both groups blocked all S-[^11^C]CGP 12388 specific binding to the perfused hearts.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20and%20PK11195%20and%20rodentia)]

Biodistribution studies in normal rats showed a high accumulation of radioactivity in the lung (10.3% injected dose (ID)/g), followed by the spleen (3.11% ID/g), heart (2.71% ID/g), kidney (1.28% ID/g) and trachea (1.25% ID/g) at 60 min after injection of S-[^11^C]CGP 12388 (6). There was a low radioactivity (0.07-0.11% ID/g) of the tracer in the brain and plasma. Pretreatment of rats with propranolol decreased significantly the accumulation of S-[^11^C]CGP 12388 in the heart, spleen and lung. PET studies showed that the lung was clearly visualized and the accumulation was blocked by pretreatment with propranolol. Time-activity curves for the lung indicated that S-[^11^C]CGP 12388 was slowly washed out (t_1/2_, 130 min) after a rapid distribution phase. Almost all the radioactivity in the heart and lung was intact S-[^11^C]CGP 12388 at 60 min post injection (8). The fraction of plasma radioactivity of intact S-[^11^C]CGP 12388 was 61% at 60 min after injection.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20and%20PK11195%20and%20%28dog%20or%20pig%20or%20rabbit%20or%20sheep%29)]

No publications are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20and%20PK11195%20and%20%28primate%20not%20human%29)]

No publications are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20and%20PK11195%20and%20human)]

Elsinga et al (9) reported a human study by administration S-[^11^C]CGP 12388 to 5 healthy volunteers on two separate days (control and pindolol pretreatment study). Heart, lung and spleen showed high uptake of radioactivity, which was strongly suppressed (68-77%) by pindolol (a β-adrenoceptor antagonist), representing binding to β-adrenoceptors. The washout rates were slow for the heart (0.0056/min), lung (0.0033/min) and spleen (0.015/min). Plasma clearance of S-[^11^C]CGP 12388 was rapid and tri-phasic (t_1/2_, 0.22, 2.51 and 101.53 min), binding to plasma proteins was low (53 ± 4%), and S-[^11^C]CGP12388 was slowly metabolized (87% intact at 10 min). S-[^11^C]CGP 12388 produced high-quality images of the human thorax.

Doze et al. (10) reported on PET studies in 6 healthy volunteers after three injections of S-[^11^C]CGP 12388 (high specific activity, low specific activity or unlabeled ligand only). Using tracer kinetic modeling, the B_max_ and K_d_ of S-[^11^C]CGP 12388 for the β-adrenoceptors in the heart were determined to be 9.74 ± 1.80 nM and 0.58 ± 0.22 nM, assuming a reaction volume of 0.15. Time-activity curves revealed the displacement of S-[^11^C]CGP 12388 by the unlabeled tracer from the β-adrenoceptors. Using the same kinetic modeling, myocardial β-adrenoceptors was investigated in 6 patients with idiopathic dilated cardiomyopathy and 6 healthy controls using S-[^11^C]CGP 12388 PET (11). The measured B_max_ of the patients (5.4 ± 1.3 pmol/g tissue) decreased 36% (P <0.005) compared to the controls (8.4 ± 1.5 pmol/g tissue).

S-[^11^C]-CGP12388 in aerosol form was administered to 8 volunteers to inhale the tracer twice, at baseline and after pretreatment with a β-adrenergic drug (salbutamol or pindolol) (12). A dynamic PET scan of the lung was followed by a whole-body scan to assess the inhaled dose at 60 min. Pretreatment consisted either of inhaled salbutamol (a β_2_-adrenoceptor agonist) (n=4, 400 μg, 20 min before the scan), or orally administered pindolol (a β-adrenoreceptor blocker) (n=4, 3 x 5 mg during a period of 16 h before PET imaging). Drug pretreatment decreased pulmonary accumulation of the radioactivity by only 7%. The agonist salbutamol accelerated the monoexponential washout of radioactivity not only in the peripheral lung (mainly alveoli), but also in the central lung (mainly airways) and in the main bronchi. An even larger increase of the washout rate was induced by the antagonist pindolol. The increased washout rates are the results of the blockade of β-adrenoceptors by salbutamol and pindolol. The washout rate of in the peripheral lung after inhalation (t_1/2_, 207 ± 48 min) was similar to that observed previously with intravenous injection (t_1/2_, 218 ± 66 min) (9). Thus, the interaction of drugs with lung β-adrenoceptors can be visualized using PET scanning and an inhaled radioligand.

Internal dosimetry data for S-[^11^C]CGP 12388 in humans are not available in the literature.

## References

1 Kopka K., Law M.P., Breyholz H.J., Faust A., Holtke C., Riemann B., Schober O., Schafers M., Wagner S. (2005). Non-invasive molecular imaging of beta-adrenoceptors in vivo: perspectives for PET-radioligands. Curr Med Chem.
2 van Waarde A., Vaalburg W., Doze P., Bosker F.J., Elsinga P.H. (2004). PET imaging of beta-adrenoceptors in human brain: a realistic goal or a mirage?. Curr Pharm Des.
3 Elsinga P.H., van Waarde A., Vaalburg W. (2004). Receptor imaging in the thorax with PET. Eur J Pharmacol.
4 Brodde, O.E., Pathophysiology of the beta-adrenoceptor system in chronic heart failure: consequences for treatment with agonists, partial agonists or antagonists? Eur Heart J, 199112 Suppl F: p. 54-62.
5 Affolter H., Hertel C., Jaeggi K., Portenier M., Staehelin M. (1985). (-)-S-[3H]CGP-12177 and its use to determine the rate constants of unlabeled beta-adrenergic antagonists. Proc Natl Acad Sci U S A.
6 Elsinga P.H., van Waarde A., Jaeggi K.A., Schreiber G., Heldoorn M., Vaalburg W. (1997). Synthesis and evaluation of (S)-4-(3-(2'-[11C]isopropylamino)-2-hydroxypropoxy) -2H-benzimidazol -2-one ((S)-[11C]CGP 12388) and (S)-4-(3-((1'-[18F]-fluoroisopropyl)amino)-2-hydroxypropoxy) -2H- benzimidazol-2-one ((S)-[18F]fluoro-CGP 12388) for visualization of beta-adrenoceptors with positron emission tomography. J Med Chem.
7 Momose M., Reder S., Raffel D.M., Watzlowik P., Wester H.J., Nguyen N., Elsinga P.H., Bengel F.M., Remien J., Schwaiger M. (2004). Evaluation of cardiac beta-adrenoreceptors in the isolated perfused rat heart using (S)-11C-CGP12388. J Nucl Med.
8 van Waarde A., Elsinga P.H., Doze P., Heldoorn M., Jaeggi K.A., Vaalburg W. (1998). A novel beta-adrenoceptor ligand for positron emission tomography: evaluation in experimental animals. Eur J Pharmacol.
9 Elsinga P.H., Doze P., van Waarde A., Pieterman R.M., Blanksma P.K., Willemsen A.T., Vaalburg W. (2001). Imaging of beta-adrenoceptors in the human thorax using (S)-[(11)C]CGP12388 and positron emission tomography. Eur J Pharmacol.
10 Doze P., Elsinga P.H., van Waarde A., Pieterman R.M., Pruim J., Vaalburg W., Willemsen A.T. (2002). Quantification of beta-adrenoceptor density in the human heart with (S)-[11C]CGP 12388 and a tracer kinetic model. Eur J Nucl Med Mol Imaging.
11 de Jong R.M., Blanksma P.K., van Waarde A., van Veldhuisen D.J. (2002). Measurement of myocardial beta-adrenoceptor density in clinical studies: a role for positron emission tomography?. Eur J Nucl Med Mol Imaging.
12 van Waarde A., Maas B., Doze P., Slart R.H., Frijlink H.W., Vaalburg W., Elsinga P.H. (2005). Positron emission tomography studies of human airways using an inhaled beta-adrenoceptor antagonist, S-11C-CGP 12388. Chest.